# Tri-gadolinium nitride PEGylated-hydroxylated endohedral metallofullerene

Chemical name: | Tri-gadolinium nitride PEGylated-hydroxylated endohedral metallofullerene
Abbreviated name: | Gd_3_N@C_80_[DiPEG_5000_(OH)_x_]
Synonym:
Agent category: | Cage molecule
Target: | Other
Target category: | Other - Retention
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal/contrast: | Gadolinium
Activation: | No
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd3N + C80)]

Fullerenes, also known as buckyballs, are spheroidal carbon cages with a molecular formula of C_2n_ (n = 30–41) and a diameter of ~1 nm (1). The high chemical stability of fullerenes can resist any potential metabolic cage-opening process and hence prevents them from degradation in various biological conditions (2). Fullerenes contain hollow interiors that can hold atoms or ions as payloads for various biomedical applications (1). For example, Gd atoms or the trimetallic nitride Gd_3_N can be trapped inside the cage to form endohedral metallofullerenes denoted as Gd@C_2n_ or Gd_3_N@C_2n_, where the “@” symbol refers to the encapsulated nature of the Gd or Gd_3_N. For the Gd@C_2n_, the encapsulation of electropositive Gd atom leads to the transfer of electrons from the Gd atom to the electronegative fullerene cage, resulting in a zwitterion [Gd^3+^@C_82_^3-^]. For Gd_3_N@C_2n_, each Gd atom shares one electron with the N atom and donates the other two electrons to the C80 cage that is in I_h_-symmetry to produce a zwitterion [Gd_3_N^6+^@C_80_^6-^] (3, 4). These endohedral metallofullerenes thus lead to the generation of a novel type of contrast agent for magnetic resonance imaging (MRI), which possesses a high biological safety in that the carbon cage completely prevents the release of toxic Gd^3+^ ions into surrounding tissues (5, 6). The surface of fullerenes can be functionalized with a variety of groups or specific ligands; i.e., the addition of hydroxyls or polyethylene glycols (PEG) substantially increases their aqueous solubility (7).

The tri-gadolinium nitride PEGylated-hydroxylated endohedral metallofullerene (Gd_3_N@C_80_[DiPEG_5000_(OH)_x_]) is a PEG_5000_-functionalized trimetallic nitride endohedral metallofullerene for in vivo MRI (2). The encapsulation of three Gd ions inside the carbon cage prevents direct coordination and exchange of water to Gd^3+^. The relaxation enhancement of Gd_3_N@C_80_[DiPEG_5000_(OH)_x_] is therefore quite different from the classic inner-sphere mechanism in conventional Gd chelates such as Gd-DOTA (1). Depending on the symmetry of Gd_3_N (pyramidal) and the C_80_ cage (icosahedral), Gd_3_N@C_80_[DiPEG_5000_(OH)_x_] can possess a permanent dipolar moment to induce an increase of T_1_ relaxivity as much as 30 times more than that of Gd-DOTA (2).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( Gd3N + C80)+AND+synthesis%0D%0A)]

Fatouros et al. described the preparation of Gd_3_N@C_80_[DiPEG_5000_(OH)_x_] in two steps (2). Initially, Gd_3_N@C_80_ was obtained by arc-vaporization of graphite rods packed with Gd_2_O_3_, Fe_x_N, and graphite powder in a Krätschmer-Huffman (K-H) electric-arc generator in a N_2_/He atmosphere (3). The obtained soot was mixed with CBr_4_ in toluene under sonication, and the resulting mixture was reacted with PEG malonate (Mw ~10,000) and 1,8-diazabicyclo[5.4.0]-undec-7-ene for 20 h under nitrogen atmosphere at room temperature (2). The produced Gd_3_N@C_80_[DiPEG_5000_(OH)_x_] was purified with silica gel column chromatography and the gadolinium content was measured with the inductively coupled plasma optical emission spectroscopy (ICP-OES).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( Gd3N + C80)+AND+%22in+vitro%22)]

The T_1_/T_2_ relaxivity of Gd_3_N@C_80_[DiPEG_5000_(OH)_x_] appeared to be dependent on concentration (2). In the low concentration range of 0.0016–0.0126 mM, the T_1_ relaxivity was 102 mM^-1^s^-1^ at 0.35 T, 143 mM^-1^s^-1^ at 2.4 T, and 32 mM^-1^s^-1^ at 9.4 T, and the corresponding T_2_ relaxivity values were 144 mM^-1^s^-1^, 222 mM^-1^s^-1^, and 137 mM^-1^s^-1^, respectively. A nonlinear relaxivity pattern was found over the concentration range of 0.0016–0.202 mM at 2.4 T. Compared to conventional MRI contrast agents such as Gd-DOTA, which has a T_1_ relaxivity value of 3.84 mM^-1^s^-1^ at 0.47 T, the T^1^ relaxivity of Gd_3_N@C_80_[DiPEG_5000_(OH)_x_] increased ~30-fold per fullerene molecule or ~10-fold per Gd ion.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( Gd3N + C80) +AND++rodentia)]

Fatouros et al. examined the relaxation enhancement of Gd_3_N@C_80_[DiPEG_5000_(OH)_x_] with in vivo MRI (2). Rats were implanted intracerebrally with glioma RT2 tumors. Fourteen days after implantation, the rats were infused with 18 μl 0.0131 mM Gd_3_N@C_80_[DiPEG_5000_(OH)_x_] through the convention-enhanced delivery (CED) procedure at a rate of 0.2 μl/min for 90 min. T_2_-Weighted images were collected with a 2.4-T imager at the end of the infusion and at 17, 18, and 19 days after tumor implantation. At 19 days after implantation, the same rat was injected intravenously with 0.2 mM gadodiamide, a conventional MRI contrast agent, to assess the tumor. The T_2_-weighted images exhibited a prolonged residence of Gd_3_N@C_80_[DiPEG_5000_(OH)_x_] within the tumor region and an improved sensitivity in tumor delineation compared to that of gadodiamide. As a control, a normal rat was infused bilaterally with 15 μl 0.0131 mM Gd_3_N@C_80_[DiPEG_5000_(OH)_x_] and 0.5 mM gadodiamide at a rate of 0.2 μl/min for 75 min. Sequential T_1_-weighted images were collected with a 2.4-T imager through the 75-min infusion phase and 100 min after infusion, which demonstrated a much slower diffusion of Gd_3_N@C_80_[DiPEG_5000_(OH)_x_] in the healthy brain tissue compared with the diffusion of gadodiamide.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( Gd3N + C80) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( Gd3N + C80) +AND+human)]

No publication is currently available.

### NIH Support

CA 119371

## References

1 Bolskar R.D. (2008). Gadofullerene MRI contrast agents. Nanomed.
2 Fatouros P.P., Corwin F.D., Chen Z.J., Broaddus W.C., Tatum J.L., Kettenmann B., Ge Z., Gibson H.W., Russ J.L., Leonard A.P., Duchamp J.C., Dorn H.C. (2006). In vitro and in vivo imaging studies of a new endohedral metallofullerene nanoparticle. Radiology.
3 Ge Z., Duchamp J.C., Cai T., Gibson H.W., Dorn H.C. (2005). Purification of endohedral trimetallic nitride fullerenes in a single, facile step. J Am Chem Soc.
4 Aihara J. (2001). Kinetic stability of metabllofullerenes as predicted by bond resonance enery model. Phys. Chem. Chem. Phys.
5 Lu J., Sabirianov R.F., Mei W.N., Gao Y., Duan C.G., Zeng X. (2006). Structural and magnetic properties of Gd3N@C80. J Phys Chem B.
6 Krause M., Dunsch L. (2005). Gadolinium nitride Gd3N in carbon cages: the influence of cluster size and bond strength. Angew Chem Int Ed Engl.
7 MacFarland D.K., Walker K.L., Lenk R.P., Wilson S.R., Kumar K., Kepley C.L., Garbow J.R. (2008). Hydrochalarones: a novel endohedral metallofullerene platform for enhancing magnetic resonance imaging contrast. J Med Chem.